# 1-[^11^C]Methylpiperidin-4-yl propionate

Chemical name: | 1-[^11^C]Methylpiperidin-4-yl propionate
Abbreviated name: | [^11^C]PMP
Synonym: | [^11^C]MP4P
Agent category: | Compound
Target: | Acetylcholinesterase (AChE)
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP)]

Acetylcholine is an endogenous neurotransmitter at cholinergic synapses and neuroeffector junctions in the peripheral and central nervous systems. It acts on nicotinic and muscarinic receptors to mediate complex functions, such as attention, memory, cognition, and consciousness. Degeneration of cholinergic neurons has been observed in several neurodegenerative disease, such as Alzheimer’s disease (AD) and Parkinson’s disease (PD), but not in vascular dementia. Acetylcholinesterase (AChE) is the enzyme that terminates cholinergic actions through the rapid hydrolysis of acetylcholine to choline and acetate. AChE is localized on both cholinergic and cholinoceptive neurons in the brain with the highest activity in the striatum, followed by the cerebellum, thalamus, and cerebral cortex (1). AChE has been a target for radioligand development as well as drug development because its levels decrease in AD (1, 2).

For measurements of AChE activity, various labeled esters of 1-methy-4-hydroxypiperidine have been designed and evaluated as acetylcholine substrate analogs (3). Two of them, N-[^11^C]methylpiperidin-4-yl acetate ([^11^C]MP4A) and 1-[^11^C]methylpiperidin-4-yl propionate ([11C]PMP), were chosen for further development as radioligands for use in positron emission tomography (PET). Each has a tertiary amine structure that makes it lipophilic; thus, it readily crosses the blood-brain barrier (BBB). [^11^C]PMP is specifically hydrolyzed by AChE (86-95% specificity) and yields a hydrophilic metabolite, N-[^11^C]methylpiperidinol ([^11^C]MP4OH), which is trapped in the brain because it cannot cross the BBB. The hydrolysis rate of MP4P is 3- to 4-fold slower than that of MP4A in rat and human brain homogenates (1), thus allowing more precise estimates of AChE activity in regions of moderate to high AChE levels. [^11^C]PMP is being developed as a PET agent for the non-invasive study of brain AChE activity in patients with AD and PD.

### Related Resource Links

- Chapters in MICAD (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=acetylcholinesterase++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=43&log$=genesensor5&logdbfrom=protein)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (AChE (http://omim.org/entry/100740))
- Clinical trials (AChE (http://www.clinicaltrials.gov/ct2/results?term=acetylcholinesterase))
- Drug information in FDA (AChE (http://google-test.fda.gov/search?q=Acetylcholinesterase+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=15&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP%20and%20synthesis)]

Snyder et al. (4) reported synthesis of [^11^C]PMP by direct N-methylation of 4-piperidinyl propionate with [^11^C]methyl trifluoromethanesulfonate at room temperature in dimethylformamide, with a radiochemical yield of 57% (end of synthesis) after high-performance liquid chromatography purification. Radiochemical purities were >99% with a specific activity of 41 GBq/mmol (1,500 Ci/mmol) and a total synthesis time of ~35 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMP%29%20and%20in%20vitro)]

Shinotoh et al. (1) reported that PMP was rapidly hydrolyzed to MP4OH and propanoic acid by rat and human brain homogenates with 95 and 86% specificity for AChE, respectively. The hydrolysis rate in human cerebral cortex (0.042 fraction/min/g/ml) is about 10% that in rat cerebral cortex (0.39 fraction/min/g/ml).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP%20and%20rodentia)]

Kilbourn et al. (5) reported that 2 min after injection in mice, [^11^C]PMP showed rapid accumulation in the brain and a regional retention of radioactivity in the striatum (12.9 ± 0.86% of injected dose (ID)/g), cortex (10.9 ± 1.31% ID/g), hippocampus (10.5 ± 1.33% ID/g), thalamus (9.53 ± 1.1% ID/g), hypothalamus (8.67 ± 1.48% ID/g), and cerebellum (7.01 ± 0.97% ID/g), reflecting known levels of AChE activity in the rodent brain. More than 95% of radioactivity in the brain was the hydrolytic metabolite, [^11^C]MP4OH. There was a gradual washout in all regions with time (up to 30 min). At 10 min after injection, the striatum/cerebellum, cortex/cerebellum, and striatum/cortex ratios were 3.06 ± 0.31, 1.1.79 ± 0.15, and 1.71 ± 0.19, respectively. On the other hand, for [^11^C]MP4A, the striatum/cerebellum, cortex/cerebellum, and striatum/cortex ratios were 1.81 ± 0.20, 1.64 ± 0.12, and 1.09 ± 0.08, respectively. Therefore, [^11^C]PMP seems to be better for discrimination among regions of high, intermediate, and low AChE activity. Retention of [^11^C]PMP radioactivity in all regions was reduced by pretreatment with 3 mg/kg diisopropylfluorophosphate (DFP), a specific irreversible AChE inhibitor. DFP pretreatment also significantly increased the proportions of intact ester in both blood and brain. Using PET scans, Shao et al. (6) estimated [^11^C]PMP hydrolysis rate constant (k_3_) values for the striatum and cortex to be 0.1009/min and 0.0453/min, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP%20and%20%28primate%20not%20human%29)]

Kilbourn et al. (5) performed [^11^C]PMP PET studies in one monkey and found rapid accumulation in the brain within minutes after injection. About 15% and 50% of the initial high uptake in the striatum and cortex, respectively, was washed out in the initial 15 min and then remained constant with a maximal striatum/cortex ratio of 2.25, compared with 1.8 with [^11^C]MP4A.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMP%20and%20human)]

Kinetic analysis of [^11^C]PMP for measurement of cerebral AChE activity has been performed with and without arterial blood sampling (7, 8). A three-compartment model with three parameters was used to measure AChE hydrolysis of the tracer (k_3_), the transport rate constant of the tracer from the blood to the brain through the BBB (K_1_), and the transport rate constant of the tracer from the brain to the blood through the BBB (k_2_). Kuhl et al. (9) studied 26 healthy controls and 14 patients with AD who had no dementia; the authors used [^11^C]PMP PET, 2-[^18^F]fluoro-2-deoxy-D-glucose (FDG), and 5-[^123^I]iodobenzovesamicol ([^123^I]IBVM) for AChE activity, glucose metabolism, and vesicular acetylcholine transporter activity, respectively. The highest uptake was in the striatum, followed by the cerebellum, pons, thalamus, occipital cortex, temporal cortex, and frontal cortex. The estimated AChE distribution in the brain of the control subjects agreed with the AChE distribution at biopsies reported by others (10, 11). There was a 30% reduction of AChE activity in the cerebral cortex of the AD patients compared with the controls. Treatment with physostigmine (an AChE inhibitor) produced little effect on the [^11^C]PMP K_1_ in the controls. In contrast, there were significant decreases in the [^11^C]PMP k_3_ of all brain regions. There was a 15% decrease in cortical [^11^C]PMP K_1_ in elderly controls compared with young controls. However, there was no correlation of [^11^C]PMP k_3_ values with age and gender. In 11 AD patients, [^11^C]PMP k_3_ correlated significantly with [^123^I]IBVM binding, but neither the [^11^C]PMP k_3_ nor [^123^I]IBVM binding correlated with FDG uptake. After treatment with donepezil (an AChE inhibitor), cerebral cortical [^11^C]PMP k_3_ inhibition in AD brain averaged 27% in 6 patients (12).

Marshall et al. (13) studied the relationship between the severity of white matter hyperintensity (WMH) and cortical AChE activity in 11 patients with parkinsonian dementia (PDem) and 14 control subjects. [^11^C]PMP k_3_ values were significantly reduced (–20%; P< 0.001) in the cortex of PDem patients (0.0185 ± 0.0019/min) compared with the controls (0.0231 ± 0.0026/min). PDem subjects had higher mean severity of WMH (+20.1%) compared with control subjects (P < 0.05). However, there was no significant correlation of cortical [^11^C]PMP AChE activity with WMH severity. Bohnen et al. (14) found that [^11^C]PMP AChE activity was significantly reduced (–11%; P < 0.05) in the cortex in patients with mild to moderate AD (0.0201 ± 0.0018/min; n = 15) compared with 12 normal controls (0.0226 ± 0.0023/min). Cortical [^11^C]PMP AChE activity was more robustly associated with functions of attention and working memory (P = 0.01) than with performance on primary memory tests in AD.

Internal dosimetry data for [^11^C]PMP in humans are not yet available in the literature

## References

1 Shinotoh H., Fukushi K., Nagatsuka S., Irie T. (2004). Acetylcholinesterase imaging: its use in therapy evaluation and drug design. Curr Pharm Des.
2 Herholz K. (2003). PET studies in dementia. Ann Nucl Med.
3 Irie T., Fukushi K., Akimoto Y., Tamagami H., Nozaki T. (1994). Design and evaluation of radioactive acetylcholine analogs for mapping brain acetylcholinesterase (AchE) in vivo. Nucl Med Biol.
4 Snyder S.E., Tluczek L., Jewett D.M., Nguyen T.B., Kuhl D.E., Kilbourn M.R. (1998). Synthesis of 1-[11C]methylpiperidin-4-yl propionate ([11C]PMP) for in vivo measurements of acetylcholinesterase activity. Nucl Med Biol.
5 Kilbourn M.R., Snyder S.E., Sherman P.S., Kuhl D.E. (1996). In vivo studies of acetylcholinesterase activity using a labeled substrate, N-[11C]methylpiperdin-4-yl propionate ([11C]PMP). Synapse.
6 Shao X., Koeppe R.A., Butch E.R., Kilbourn M.R., Snyder S.E. (2005). Evaluation of 18F-labeled acetylcholinesterase substrates as PET radiotracers. Bioorg Med Chem.
7 Koeppe R.A., Frey K.A., Snyder S.E., Meyer P., Kilbourn M.R., Kuhl D.E. (1999). Kinetic modeling of N-[11C]methylpiperidin-4-yl propionate: alternatives for analysis of an irreversible positron emission tomography trace for measurement of acetylcholinesterase activity in human brain. J Cereb Blood Flow Metab.
8 Sato K., Fukushi K., Shinotoh H., Nagatsuka S., Tanaka N., Aotsuka A., Ota T., Shiraishi T., Tanada S., Iyo M., Irie T. (2004). Evaluation of simplified kinetic analyses for measurement of brain acetylcholinesterase activity using N-[11C]Methylpiperidin-4-yl propionate and positron emission tomography. J Cereb Blood Flow Metab.
9 Kuhl D.E., Koeppe R.A., Minoshima S., Snyder S.E., Ficaro E.P., Foster N.L., Frey K.A., Kilbourn M.R. (1999). In vivo mapping of cerebral acetylcholinesterase activity in aging and Alzheimer's disease. Neurology.
10 Atack J.R., Perry E.K., Bonham J.R., Candy J.M., Perry R.H. (1986). Molecular forms of acetylcholinesterase and butyrylcholinesterase in the aged human central nervous system. J Neurochem.
11 Reinikainen K.J., Riekkinen P.J., Paljarvi L., Soininen H., Helkala E.L., Jolkkonen J., Laakso M. (1988). Cholinergic deficit in Alzheimer's disease: a study based on CSF and autopsy data. Neurochem Res.
12 Kuhl D.E., Minoshima S., Frey K.A., Foster N.L., Kilbourn M.R., Koeppe R.A. (2000). Limited donepezil inhibition of acetylcholinesterase measured with positron emission tomography in living Alzheimer cerebral cortex. Ann Neurol.
13 Marshall G.A., Shchelchkov E., Kaufer D.I., Ivanco L.S., Bohnen N.I. (2006). White matter hyperintensities and cortical acetylcholinesterase activity in parkinsonian dementia. Acta Neurol Scand.
14 Bohnen N.I., Kaufer D.I., Hendrickson R., Ivanco L.S., Lopresti B., Davis J.G., Constantine G., Mathis C.A., Moore R.Y., DeKosky S.T. (2005). Cognitive correlates of alterations in acetylcholinesterase in Alzheimer's disease. Neurosci Lett.